# ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-1,4,7-triacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu
Abbreviated name: | ^64^Cu-DO3A-(GSG)-KCCYSL
Synonym:
Agent category: | Peptide
Target: | Epidermal growth factor receptor-2 (EGFR-2, HER2)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa), and it is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells, such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAbs, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A setapeptide sequence consisting of Lys-Cys-Cys-Tyr-Ser-Leu (KCCYSL) was identified using phage display screening to bind specifically to the extracellular domain of HER2 (17). ^111^In-1,4,7,10-Tetraazacyclododecane-1,4,7-tris-acetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^111^In-DOTA-(GSG)-KCCYSL (http://www.ncbi.nlm.nih.gov/books/NBK23014/)) was evaluated in nude mice bearing human breast tumor xenografts for single-photon emission computed tomography imaging (18). For positron emission tomography (PET), Kumar et al. (19) prepared ^64^Cu-1,4,7,10-tetraazacyclododecane-1,4,7-triacetic acid-(Gly-Ser-Gly)-Lys-Cys-Cys-Tyr-Ser-Leu (^64^Cu-DO3A-(GSG)-KCCYSL) for imaging of HER2 expression in breast tumors.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20synthesis)]

GSG-KCCYSL peptides were prepared with solid-phase peptide synthesis (19). The metal chelator DOTA was coupled to the amino terminus of GSG-KCCYSL with solid-phase synthesis. DO3A-(GSG)-KCCYSL was purified with high-performance liquid chromatography (HPLC). The chemical purity of DO3A-(GSG)-KCCYSL was 98%. DO3A-(GSG)-KCCYSL (36.6 nmol) was mixed with 29.6 MBq (0.80 mCi) ^64^Cu in ammonium acetate (pH 5.5) and incubated for 90 min at 85°C. ^64^Cu-DO3A-(GSG)-KCCYSL was purified with HPLC, with >98% radiochemical purity and 55% labeling yield. ^64^Cu-DO3A-(GSG)-KCCYSL was stable in mouse serum at 37°C after up to 2 h of incubation with some degradation at 4–24 h. The specific activity of ^64^Cu-DO3A-(GSG)-KCCYSL was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20in%20vitro)]

Kumar et al. (19) performed in vitro binding assays of ^64^Cu-DO3A-(GSG)-KCCYSL binding to human MDA-MB-435 breast carcinoma cells that express HER2 receptors. ^nat^Cu-DO3A-(GSG)-KCCYSL exhibited a IC_50_ value of 42 ± 10 nM (n = 3). ^64^Cu-DO3A-(GSG)-KCCYSL accumulated in MDA-MB-435 cells in a time-dependent manner at 37°C with a plateau at 45 min, whereas little radioactivity was observed in normal human mammary epithelial cells (184A1) that express low levels of HER2 receptors. ^64^Cu-DO3A-(GSG)-KCCYSL was stable in mouse serum at 37°C after up to 2 h of incubation with some degradation at 4–24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20rodentia)]

Kumar et al. (19) performed ex vivo biodistribution studies with 0.185 MBq (5 μCi) ^64^Cu-DO3A-(GSG)-KCCYSL in SCID mice (n = 3/group) bearing MDA-MB-435 xenografts at 0.5, 1, 2, and 4 h after injection. The tumor accumulation of radioactivity at 0.5 h after injection was 0.91 ± 0.12% injected dose/gram (ID/g) and decreased to 0.45 ± 0.20% ID/g at 4 h. High accumulation levels were observed in the kidneys (4.27 ± 0.84% ID/g), liver (1.68 ± 0.42% ID/g), and lung (0.96 ± 0.15% ID/g) at 2 h after injection. The tumor/blood, tumor/muscle, and tumor/liver ratios were 2.7, 9.0, and 0.3 at 2 h after injection, respectively. Pretreatment (10 min) with ^nat^Cu-DO3A-(GSG)-KCCYSL (76 nmol/mouse) inhibited the tumor radioactivity by 47% at 2 h after injection. Little inhibition was observed in the normal tissues. In comparison, ^64^Cu-DO3A-(GSG)-KCCYSL exhibited a higher retention in the liver and lower tumor/nontarget tissue ratios than ^64^Cu-NO2A-(GSG)-KCCYSL, which exhibited liver accumulation of 0.48 ± 0.05% ID/g and tumor/blood, tumor/muscle, and tumor/liver ratios of 7.6, 10.7, and 1.3 at 2 h after injection, respectively.

PET analysis was performed in SCID mice (the number of mice was not reported) bearing the MDA-MB-435 tumors at 2 h after injection of 12 MBq (0.32 mCi) ^64^Cu-DO3A-(GSG)-KCCYSL (19). The tumors were clearly visualized along with the kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=KCCYSL%20and%20human)]

No publication is currently available.

## NIH support

P50 CA103130-01, IR21 CA137239-01A1, 2 R01 CA093375

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Karasseva N.G., Glinsky V.V., Chen N.X., Komatireddy R., Quinn T.P. (2002). Identification and characterization of peptides that bind human ErbB-2 selected from a bacteriophage display library. J Protein Chem.
18 Deutscher S.L., Figueroa S.D., Kumar S.R. (2009). In-labeled KCCYSL peptide as an imaging probe for ErbB-2-expressing ovarian carcinomas. J Labelled Comp Radiopharm.
19 Kumar S.R., Gallazzi F.A., Ferdani R., Anderson C.J., Quinn T.P., Deutscher S.L. (2010). In vitro and in vivo evaluation of Cu-radiolabeled KCCYSL peptides for targeting epidermal growth factor receptor-2 in breast carcinomas. Cancer Biother Radiopharm.